# Cys-Arg-Glu-Lys-Ala-superparamagnetic iron oxide-Cy7 nanoparticles

Chemical name: | Cys-Arg-Glu-Lys-Ala-superparamagnetic iron oxide-Cy7 nanoparticles
Abbreviated name: | CREKA-SPIO-Cy7
Synonym:
Agent Category: | Peptide
Target: | Clotted plasma proteins
Target Category: | Binding
Method of detection: | Magnetic resonance imaging (MRI), optical near-infrared (NIR) fluorescence
Source of signal/contrast: | Iron oxide, Cy7
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CREKA+nanoparticle)]

Optical fluorescence imaging is increasingly being used to obtain images of biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in small animals. The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in magnetic resonance imaging (MRI), though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies (3).

A multimodal nanoparticle probe that consists of a contrast agent and a NIR fluorochrome may provide consistent imaging information. SPIO is composed of iron nanoparticles that are 4–6 nm diameter with a hydrodynamic diameter with dextran coating of 50 nm. SPIO nanoparticles can be internalized by RES cells and have long circulating times within an animal body. The accumulation of nanoparticles in cells causes a reduction in signal intensity with T2-weighted (T2*W) spin-echo pulse sequences. NIR fluorochromes (e.g., Cy5.5) provide an improved optical (NIR) signal from tissue. CLIO-Cy5.5 has been developed as a probe for multimodality imaging in small animals (4).

A meshwork of clotted proteins that has been identified in tumor stroma and vessels is absent in normal tissues (5, 6). The tumor-homing peptide Cys-Arg-Glu-Lys-Ala (CREKA) was identified with phage display screening in tumor-bearing mice with minimal binding to normal vessels (7). CREKA was identified as a ligand that bound to the meshwork of clotted proteins in the tumor stroma and blood vessels. CREKA was conjugated to SPIO labeled with Cy7 (CREKA-SPIO-Cy7) to study in vivo biodistribution of the nanoparticles in tumor-bearing mice. CREKA-SPIO-Cy7 is a multimodal imaging agent that consists of SPIO nanoparticles (MRI) with attachment of CREKA and Cy7 (NIR).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CREKA+nanoparticle+synthesis)]

Simberg et al. described the synthesis of CREKA-SPIO-Cy7 nanoparticles (7). Cy7 was conjugated to amino-SPIO dextran-coated nanoparticles (~50 nm in diameter) via reaction with Cy7-N-hydroxysuccinimide, followed by reaction with a bifunctional linker N-[a-maleimidoacetoxy]succinimide ester and CREKA to form CREKA-SPIO-Cy7 nanoparticles. The multimodal CREKA-SPIO-Cy7 had ~2,000 Cy7 molecules and ~8,000 peptides per nanoparticle. The extinction coefficient of the Cy7 dye is ~100,000 cm^-1^M^-1^. The quantum yield is ~0.5. The absorption maximum of the Cy7 dye is 740–760 nm, and the emission maximum is 770–790 nm. Fluorescein was used instead of Cy7 for intravital fluorescence microscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CREKA+nanoparticle+in+vitro)]

Simberg et al. (7) performed clot-binding assays with fluorescein-labeled CREKA-SPIO using murine and human plasma clots. Using fluorescence microscopy, CREKA-SPIO was found to bind to the clots, and CREKA inhibited the binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CREKA+nanoparticle+rodentia)]

Simberg et al. (7) performed in vivo confocal fluorescence microscopy in nude mice bearing MDA-MB-435 breast cancer xenografts after injection of CREKA-SPIO nanoparticles (1–4 mg/kg Fe). Little accumulation was observed in the tumors, whereas the RES tissues exhibited a high accumulation of CREKA-SPIO nanoparticles at 5–6 h. However, depletion of RES macrophages in the liver with clodronate- or Ni-liposomes prolonged the circulation of CREKA-SPIO five-fold in the blood and greatly increased the accumulation of CREKA-SPIO nanoparticles in the tumor blood vessels as compared with saline pretreatment. Less accumulation was observed in the liver after Ni-liposomal treatment. The iron content was ~six-fold greater in tumor vessels pretreated with Ni-liposomes. Up to 20% of the tumor vessel lumens were filled with fluorescence masses, which also stained positive for fibrin. Furthermore, no co-localization between fibrin and CREKA-SPIO was observed in the liver blood vessels. Little tumor accumulation was observed with control SPIO. Pretreatment with heparin, a strong clotting inhibitor, reduced tumor accumulation of CREKA-SPIO by >50%. Whole-body NIR imaging scans revealed a strong signal enhanced by CREKA-SPIO-Cy7 in the tumors and liver. However, only the tumor signal was inhibited by >50% with heparin pretreatment. MRI and CREKA blocking studies were not performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CREKA+nanoparticle+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CREKA+nanoparticle+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CREKA+nanoparticle+human)]

No publication is currently available.

## NIH Support

CA119355, CA099258

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
4 Josephson L., Kircher M.F., Mahmood U., Tang Y., Weissleder R. (2002). Near-infrared fluorescent nanoparticles as combined MR/optical imaging probes. Bioconjug Chem.
5 Dvorak H.F., Senger D.R., Dvorak A.M., Harvey V.S., McDonagh J. (1985). Regulation of extravascular coagulation by microvascular permeability. Science.
6 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
7 Simberg D., Duza T., Park J.H., Essler M., Pilch J., Zhang L., Derfus A.M., Yang M., Hoffman R.M., Bhatia S., Sailor M.J., Ruoslahti E. (2007). Biomimetic amplification of nanoparticle homing to tumors. Proc Natl Acad Sci U S A.